# 2-(4-Iodo-2,5-dimethoxyphenyl)-N-(2-[^11^C]methoxybenzyl)ethanamine

Chemical name: | 2-(4-Iodo-2,5-dimethoxyphenyl)-N-(2-[^11^C]methoxybenzyl)ethanamine
Abbreviated name: | [^11^C]CIMBI-5
Synonym:
Agent category: | Compound
Target: | 5-HT_2A_ serotonin receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[P ubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-5)]

Serotonin (5-hydroxytryptamine, 5-HT) has diverse physiological roles as a neurotransmitter in the central nervous system (1). It is involved in the regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, obsessive-compulsive disorder, and schizophrenia (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are three receptor subtypes within the G-protein–coupled 5-HT_2_ receptor family: 5-HT_2A_, 5-HT_2B_, and 5-HT_2C_.

5-HT_2A_ receptors are abundantly present in the cerebral cortex, basal forebrain, hippocampus, amygdala, dorsal thalamus, hypothalamus, superior colliculus, substantia nigra, pedunculopontine nucleus, legmental area, and myelencephalon (5). 5-HT_2A_ receptors are involved in mediation of normal and psychotic states, working memory, regulation of GABAergic and cholinergic neuronal cells, sleep, peripheral pain, and cardiovascular functions. 5-HT_2B_ receptors are found mainly in several peripheral tissues, such as the stomach, intestine, pulmonary smooth muscle, and myocardium. In the brain, 5-HT_2B_ receptors are found in discrete nuclei of the cerebellum, lateral septum, dorsal hypothalamus, dorsal raphe, and amygdala. 5-HT_2C_ receptors are found in the choroid plexus, substantia nigra, globus pallidus, and ventromedial thalamus. 5-HT_2A_ receptors are implicated in several psychiatric disorders, such as schizophrenia, depression, and obsessive-compulsive disorder. Thus, there is a need for selective ligands to investigate the pharmacological role of 5-HT_2A_ receptors.

There have been several studies to develop specific 5-HT_2A_ radioligands, such as [^11^C]ketanserin (6), [^18^F]spiperone (7), [^11^C]methylspiperone ([^11^C]NMSP), and [^18^F]setoperone [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-setoperone%5BAll%20Fields%5D)], for positron emission tomography (8) imaging. However, none of these ligands has proven to be specific for 5-HT_2A_ receptors because these compounds also bind to other receptors, such as dopamine receptors and the 5-HT_1_ receptor subtypes. Altanserin, a fluorobenzoyl derivative related to ketanserin, was reported to be a potent antagonist of 5-HT_2A_ receptors with >100-fold selectivity over D_2/3_ receptors, 5-HT_1A_, 5-HT_6_, and 5-HT_7_ (9, 10). This led to the development of 3-{2-[4-(4-[^18^F]fluorobenzoyl)-1-piperidyl]ethyl}-2-sulfanyl-3H-quinazolin-4-one ([^18^F]altanserin (http://www.ncbi.nlm.nih.gov/books/NBK23366/)) as a useful tool for 5-HT_2A_ receptor PET imaging in vivo (11). 5-HT_2A_ antagonists bind to the total pool of receptors, whereas 5-HT_2A_ agonists bind only to the high-affinity functional state of the receptor but may be more important in disease states because the high affinity sites are the ones that transmit the intracellular signals. Furthermore, 2-(4-Iodo-2,5-dimethoxyphenyl)-N-(2-[^11^C]methoxybenzyl)ethanamine ([^11^C]CIMBI-5), a potent and selective 5-HT_2A_ agonist, has been developed as a tool for studying 5-HT_2A_ agonist binding in the brain (12).

### Related Resource Links:

- Chapters in MICAD (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT2A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/gene/3356))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/omim/182135))
- Clinical trials (5-HT_2A_ (http://www.clinicaltrials.gov/ct2/results?term=5-HT2A))
- Drug information in Food and Drug Administration (5-HT_2A_ (http://google2.fda.gov/search?q=5-HT2a&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-5%20and%20synthesis)]

Ettrup et al. (12) reported a two-step reaction synthesis of [^11^C]CIMBI-5 by reacting [^11^C]methyl triflate with the Boc-protected precursor, followed by acid hydrolysis. [^11^C]CIMBI-5 was purified with column chromatography. Specific activities were 64–355 GBq/μmol (1.7–9.6 Ci/μmol) at the end of synthesis with a radiochemical purity >97%. The total synthesis time was 40–50 min. The lipophilicity (cLogD_7.4_) was calculated to be 3.21. The radiochemical yield was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-5%20and%20in%20vitro)]

CIMBI-5 has been reported to have high binding affinity for the 5-HT_2A_ receptor. Ettrup et al. (12) reported K_i_ values of 2.2, 2.3, 7.0, 58, and 85 nM for 5-HT_2A_, 5-HT_2B_, 5-HT_2C_, 5-HT_6_, and 5-HT_1A_ receptors, respectively. CIMBI-5 exhibited at least a 30-fold lower affinity for a variety of receptors. CIMBI-5 was found to induce phosphoinositide hydrolysis in GF62 cells overexpressing the 5-HT_2A_ receptor with an EC_50_ of 1.02 nM. These data demonstrate that CIMBI-5 is a specific and selective 5-HT_2A_ agonist.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-5%20and%20rodentia)]

Ex vivo biodistribution studies in rats (n = 2–4/group) showed a moderate accumulation of radioactivity in the frontal cortex at 5, 15, 30, 45, and 60 min after injection of 4 MBq/kg (0.11 mCi/kg) [^11^C]CIMBI-5 (12). Accumulation of the tracer in the frontal cortex peaked at 30 min (specific binding ratio (SBR, (region of interest – cerebellum)/cerebellum) = 0.77, using the cerebellum as a reference), followed by a slow decrease of radioactivity to an SBR of 0.5 at 60 min. The accumulation in the cerebellum was lower than in the frontal cortex and paralleled the plasma time–activity curve. Pretreatment with 1 mg/kg ketanserin 45 min before [^11^C]CIMBI-5 injection reduced the SBR to 0.076 at 30 min after injection (P < 0.0001).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-5%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Ettrup et al. (12) performed PET imaging studies in six female Danish Landrace pigs with injection of ~238 MBq (6.4 mCi) [^11^C]CIMBI-5. [^11^C]CIMBI-5 exhibited high cortical accumulation, moderate accumulation in the striatum and thalamus, and low accumulation in the cerebellum. The standard uptake values at 80 min after injection were 0.8 g/ml and 0.5 g/ml for the frontal cortex and cerebellum, respectively. Pretreatment with ketanserin reduced the standard uptake value at the same time point to 0.5 g/ml in the frontal cortex with little effect on the cerebellum. Kinetic modeling with the simplified reference tissue model (SRTM) showed that the cortical nondisplaceable binding potential (BP_ND_) value was 0.46 ± 0.11 (n = 5); this value decreased to 0.11 ± 0.06 (n = 3) with ketanserin pretreatment. One-tissue (BP_ND_ = 0.57) and two-tissue (BP_ND_ = 0.61) compartment models showed similar baseline cortical BP_ND_ values. As a comparison, [^18^F]altanserin showed a cortical SRTM BP_ND_ value of 0.47 ± 0.10. [^11^C]CIMBI-5 was >90% intact in the frontal cortex and cerebellum at 25 min after injection and ~18% intact in the plasma with two less lipophilic metabolites.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-5%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-5%20and%20human)]

No publication is currently available.

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Leysen J.E. (2004). 5-HT2 receptors. Curr Drug Targets CNS Neurol Disord.
6 Dewey S.L., Smith G.S., Logan J., Brodie J.D. (1993). Modulation of central cholinergic activity by GABA and serotonin: PET studies with 11C-benztropine in primates. Neuropsychopharmacology.
7 Shiue C.Y., Fowler J.S., Wolf A.P., Watanabe M., Arnett C.D. (1985). Syntheses and specific activity determinations of no-carrier-added (NCA) F-18-labeled butyrophenone neuroleptics--benperidol, haloperidol, spiroperidol, and pipamperone. J Nucl Med.
8 Gao X., Yang L., Petros J.A., Marshall F.F., Simons J.W., Nie S. (2005). In vivo molecular and cellular imaging with quantum dots. Curr Opin Biotechnol.
9 Leysen, J., Use of 5-HT receptor agonists and antagonists for the characterization of their respective recptor sites. In: A.B. Boulton, G.B. Baker and A.V. Jurio Editors, Drugs as Tools in Neurotransmitter Research. Neuromethods The Human Press, Clifton, NJ 1989: p. 299-341.
10 Tan P.Z., Baldwin R.M., Van Dyck C.H., Al-Tikriti M., Roth B., Khan N., Charney D.S., Innis R.B. (1999). Characterization of radioactive metabolites of 5-HT2A receptor PET ligand [18F]altanserin in human and rodent. Nucl Med Biol.
11 Lemaire C., Cantineau R., Guillaume M., Plenevaux A., Christiaens L. (1991). Fluorine-18-altanserin: a radioligand for the study of serotonin receptors with PET: radiolabeling and in vivo biologic behavior in rats. J Nucl Med.
12 Ettrup A., Palner M., Gillings N., Santini M.A., Hansen M., Kornum B.R., Rasmussen L.K., Nagren K., Madsen J., Begtrup M., Knudsen G.M. (2010). Radiosynthesis and evaluation of 11C-CIMBI-5 as a 5-HT2A receptor agonist radioligand for PET. J Nucl Med.